# Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-sr39tk

Chemical name: | Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-sr39tk
Abbreviated name: | AdTSTA-sr39tk
Synonym:
Agent Category: | Protein (virus)
Target: | Androgen receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^FHBG
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is current available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AdTSTA-sr39tk)]

Adenoviruses (Ads) comprise a non-enveloped icosahedral protein shell (capsid) 70–100 nm in diameter surrounding an inner vial genome core (1). Human Ads consist of 51 distinct serotypes that are classified into six subgroups (species) designated A–F (2). Some serotypes such as serotypes 2 (Ad2) and 5 (Ad5) of species C only induce a mild, non-oncogenic respiratory infection, making them suitable for development of Ad-based vaccines and gene delivery vehicles for systematic administrations (1). Their core genome, a linear, double-stranded DNA of ~36 kb, contains five early transcription units (E1A, E1B, E2, E3, and E4), four intermediate units (IVA2, IX, VAI, and VAII), and one later transcription unit (2). The functions in the early transcription regions have been well identified: E1A activates cell cycles and initiates DNA replication; E1B blocks apoptosis induced by E1A activity; E2 facilitates viral DNA replication; E3 modulates host immune responses; and E4 regulates DNA replication, mRNA transport, and apoptosis (3). As a gene delivery vehicle, the genome core in Ad2 or Ad5 is usually modified with recombinant transcription activators (RTAs), in which foreign DNA with a size of up to 7.5 kb can be inserted in the deleted E1 or E3 regions in the Ads (4). Such genetic modification can incorporate ligands that can recognize specific cellular receptors and/or block the adenoviral naïve receptor (coxsackie-adenovirus receptor (CAR)), so that their tissue specificity is enhanced significantly. For example, the gene for the androgen receptor (AR) regulates the growth of prostate epithelial cells, induces the expression of prostate-specific antigen (PSA), and controls the growth of prostate cancer in the early phase. The AR gene can be introduced to the adenoviral genome to target AR-responsive prostate cancer or metastasis (5). Furthermore, reporter genes such as firefly luciferase (Fluc) (6) can be included for in vivo optical imaging, or suicide genes such as herpes simplex virus type 1-thymidine kinase (HSV1-TK, also a reporter gene for positron emission tomography (PET)), can be used for therapeutic applications (7).

HSV1-TK is a homodimer composed of two 376-residue subunits, and it functions as a key enzyme in the pyrimidine-salvage pathway to catalyze the phosphorylation of thymidine (dT) to thymidine monophosphate (dTMP) in the presence of ATP and Mg^2+^ (7). Unlike mammalian thymidine kinases, HSV1-TK can efficiently phosphorylate substrates such as acycloguanosines and uracils (8). Thus, radiolabeled acycloguanosines such as 9-(4-[^18^F]fluoro-3-hydroxymethylbutyl)guanine ([^18^F]FHBG, [^18^F]FPCV) or uracils such as 2’-fluoro-2’-deoxy-1-β-D-arabino-furanosyl-5-iodo-uracil ([^131^I]FIAU) are used as HSV1-TK imaging probes for positron emission tomography (PET) or single-photon emission tomography (SPECT). As a mutant of HSV1-TK, HSV1-sr39tk has five nonpolar amino acids being replaced at its active site: L159I, I160F, F161L, A162F, and L163M (9). Such remodeling in the active site leads to a substantial increase in the binding affinity to acycloguanosines; i.e., the 50% inhibition concentration of ganciclovir reduces ~300-fold. This also increases the imaging detection sensitivity; i.e., a more than two-fold enhancement has been observed in detection of [^18^F]FHBG with HSV1-sr39tk compared to that with HSV1-TK, which provides an efficient gene-reporter probe combination (HSV1-sr39tk-[^18^F]FHBG) for PET imaging (8).

The transcriptional activity of adenoviral genes can be amplified several orders of magnitude with the use of the GAL4-VP2 fusion protein, where GAL4 is a DNA-binding domain (147 amino acids) and VP2 is a two-tandem repeat of the herpes simplex virus VP16 acidic activation domain (78 amino acids) (10). The two-step transcriptional amplification (TSTA) system is a novel recombinant transcription activation approach for designing a PSA promoter/enhancer, which can provide as high as ~800-fold enhancement in transcription activity compared with its conventional analog (11, 12). The TSTA system is composed of two parts in general; i.e., an activator PBC-VP2 that contains a PSA promoter with a duplicated ARE4 enhancer core (each core has four binding sites for AR) to control the expression of the chimeric protein GAL4-VP2 and provide cell-specific binding, and the reporter (GAL4)_5_-sr39tk (G5-sr39tk), which contains a reporter with five GAL4 repeats to generate a GAL4-responsive sr39tk (13). The two parts are linked in a head-to-head orientation and are inserted into the E1 region of Ad5 to produce Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-sr39tk (AdTSTA-sr39tk), a reporter gene for PET imaging of AR-responsive PSA in vivo. Such a construct can provide ~12-fold amplification (12) via two steps: the PSA regulates the expression of the potent transcription activator GAL4-VP2, which in turn activates the GAL4-responsive reporter gene sr39tk. AdTSTA-sr39tk can function effectively as a gene delivery vehicle and as a lymphotropic agent in prostate cancer and metastasis in vivo (13, 14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(AdTSTA-sr39tk)+AND+synthesis%0D%0A)]

The preparation of AdTSTA-sr39tk was conducted in several steps (12, 13, 15). The commercial plasmid pBS II SK+ was used as the starting baseline construct pPSE (12). A NotI-flanked PSA enhancer/promoter expression cassette derived from plasmid PSAR2.4k-PCPSA-P-Lux was inserted into the pPSE to produce PSE. The synthetic ARE4 element that contained four key ARE elements was used to generate a duplicated enhancer core (15). The insertion of this duplicated core (C)in the PSE replaced the sequence between -3935 and -2855 in the PSE to produce a plasmid vector PBC. Then a GAL-VP2 fragment was inserted into PBC followed by the creation of a unique NotI site. A NotI fragment, which contained both the PBC promoter and GAL-VP2 gene, was excised from the obtained plasmid PBC-VP2 and cloned into the NotI site of G5-sr39tk to generate the vector PBC-VP2G5-sr39tk (11, 13). A SalI-Notl fragment containing the PBC-VP2G5-sr39tk fragment was derived from the resulting PBC-VP2G5-sr39tk and excised by NotI and partial SalI digestion (13). The produced expression cassette PBC-VP2G5-sr39tk was inserted into the SalI-NotI site of the commercial vector pShuttle, which was then incorporated into the commercial Ad vector AdEasy through homologous recombination to produce AdTSTA-sr39tk. The virus was propagated in 293 cells, purified on a CsCl gradient, and titered with plaque assays on 293 monolayers.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(AdTSTA-sr39tk)+AND+%22in+vitro%22)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(AdTSTA-sr39tk) +AND++rodentia)]

Burton et al. examined the movement of AdTSTA-sr39tk to lymph nodes in vivo (14). SCID/Beige (natural killer–deficient) mice were implanted with LAPC-9-VEGF-C tumor cells on the right shoulder, and the tumors were allowed to grow for 30 d. After resection of the tumor, the mice were injected with 1 × 10^8^ pfu AdTSTA-sr39tk in 30 μl phosphate-buffered saline in their forepaws followed by an intravenous injection of ~250 μCi [^18^F]FHBG. Micro-PET images were collected 1 h later for 20 min followed by imaging with micro-CT for 7 min. A positive [^18^F]FHBG PET signal was observed in the ipsilateral but not in contralateral axillary lymph nodes. Tumor cell-localized expression of sr39tk was found in the respective lymph nodes by immunohistological staining. Burton et al. then incorporated AdTSTA-sr39tk in the lymphoscintigraphy to assess lymph node metastases (14). Mice (n = 6) were implanted with Renilla luciferase (RL)-labeled tumors (LAPC-9-C-GFP-RL; ~1.0 cm in diameter) on their right upper back, and they also received a tumor-directed injection of 5 × 10^8^ pfu AdTSTA-sr39tk. One hour after intravenous injection of ~250 μCi [^18^F]FHBG, PET/CT images were collected. Robust [^18^F]FHBG PET signals were detected in the tumor and the draining axillary lymph nodes. Immediately after the PET/CT imaging, ipsilateral and contralateral lymph nodes were removed for quantification of their radioactivity and RL bioluminescence. The radioactivity in the ipsilateral lymph nodes was found to be twice as high as the radioactivity in the contralateral lymph nodes. Also, the measurement of RL bioluminescence in the isolated lymph nodes confirmed the presence of disseminated tumor cells. These results exhibited an effective movement of AdTSTA-sr39tk to the sentinel lymph node and allowed for direct detection of nodal metastasis with PET.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(AdTSTA-sr39tk) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(AdTSTA-sr39tk) +AND+human)]

No publication is currently available.

### NIH Support

CA 82214, CA 09056, CA 86306, CA 92131, CA101904, CA 92865, GM 08652

## References

1 Douglas J.T. (2007). Adenoviral vectors for gene therapy. Mol Biotechnol.
2 Majhen D., Ambriovic-Ristov A. (2006). Adenoviral vectors--how to use them in cancer gene therapy?. Virus Res.
3 Kuhlmann K.F., Gouma D.J., Wesseling J.G. (2008). Adenoviral gene therapy for pancreatic cancer: where do we stand?. Dig Surg.
4 Nettelbeck D.M., Jerome V., Muller R. (2000). Gene therapy: designer promoters for tumour targeting. Trends Genet.
5 Zhang L., Johnson M., Le K.H., Sato M., Ilagan R., Iyer M., Gambhir S.S., Wu L., Carey M. (2003). Interrogating androgen receptor function in recurrent prostate cancer. Cancer Res.
6 Sato M., Johnson M., Zhang L., Zhang B., Le K., Gambhir S.S., Carey M., Wu L. (2003). Optimization of adenoviral vectors to direct highly amplified prostate-specific expression for imaging and gene therapy. Mol Ther.
7 Johnson M., Sato M., Burton J., Gambhir S.S., Carey M., Wu L. (2005). Micro-PET/CT monitoring of herpes thymidine kinase suicide gene therapy in a prostate cancer xenograft: the advantage of a cell-specific transcriptional targeting approach. Mol Imaging.
8 Gambhir S.S., Bauer E., Black M.E., Liang Q., Kokoris M.S., Barrio J.R., Iyer M., Namavari M., Phelps M.E., Herschman H.R. (2000). A mutant herpes simplex virus type 1 thymidine kinase reporter gene shows improved sensitivity for imaging reporter gene expression with positron emission tomography. Proc Natl Acad Sci U S A.
9 Black M.E., Kokoris M.S., Sabo P. (2001). Herpes simplex virus-1 thymidine kinase mutants created by semi-random sequence mutagenesis improve prodrug-mediated tumor cell killing. Cancer Res.
10 Sadowski I., Ma J., Triezenberg S., Ptashne M. (1988). GAL4-VP16 is an unusually potent transcriptional activator. Nature.
11 Zhang L., Adams J.Y., Billick E., Ilagan R., Iyer M., Le K., Smallwood A., Gambhir S.S., Carey M., Wu L. (2002). Molecular engineering of a two-step transcription amplification (TSTA) system for transgene delivery in prostate cancer. Mol Ther.
12 Iyer M., Wu L., Carey M., Wang Y., Smallwood A., Gambhir S.S. (2001). Two-step transcriptional amplification as a method for imaging reporter gene expression using weak promoters. Proc Natl Acad Sci U S A.
13 Sato M., Johnson M., Zhang L., Gambhir S.S., Carey M., Wu L. (2005). Functionality of androgen receptor-based gene expression imaging in hormone refractory prostate cancer. Clin Cancer Res.
14 Burton J.B., Johnson M., Sato M., Koh S.B., Mulholland D.J., Stout D., Chatziioannou A.F., Phelps M.E., Wu H., Wu L. (2008). Adenovirus-mediated gene expression imaging to directly detect sentinel lymph node metastasis of prostate cancer. Nat Med.
15 Wu L., Matherly J., Smallwood A., Adams J.Y., Billick E., Belldegrun A., Carey M. (2001). Chimeric PSA enhancers exhibit augmented activity in prostate cancer gene therapy vectors. Gene Ther.
16 Figures, Tables and Boxes Appendix (do not delete)